# 2-(5-[^11^C]Methyl-hexahydro-pyrrolo[3,4-c]pyrrol-2-yl)-xanthene-9-one

Chemical name: | 2-(5-[^11^C]Methyl-hexahydro-pyrrolo[3,4-c]pyrrol-2-yl)-xanthene-9-one
Abbreviated name: | [^11^C]A-844606
Synonym:
Agent category: | Compound
Target: | Neuronal α7 nicotinic acetylcholine receptor (nAChR)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=A-844606)]

Neuronal α4β2 nicotinic cholinergic receptors (nAChRs) are part of a heterogeneous family of ligand-gated ion channels expressed in the central nervous system, where their activation by acetylcholine and nicotine causes a rapid increase in cellular permeability to ions, such as Na^+^ and Ca^2+^ (1-3). Nicotinic receptors exist as pentamers (homomeric or heteromeric) in various brain regions and ganglia. There are nine subtypes of ligand-binding α receptors (α2 to α10) and four subtypes of structural β receptors (β2 to β5). nAChRs have been found to be involved in cognitive processes such as learning memory and control of movement in normal subjects. nAChR dysfunction has been implicated in a number of human diseases such as schizophrenia, Huntington's disease, Alzheimer's disease, and Parkinson's disease. nAChRs also play a significant role in nicotine addiction and other health problems associated with tobacco smoking.

3-[2(S)-2-Azetidinylmethoxy]pyridine (A-85380) is a highly potent and selective α4β2 nAChR agonist with subnanomolar affinity (4, 5). 6-[^18^F]Fluoro-A-85380 and 2-[^18^F]fluoro-A-85380 have been studied in humans as positron emission tomography (6) agents for α4β2 nAChR imaging in the brain for studying neuropsychiatric disorders. A-85380 has also been labeled as 5-[^123^I]iodo-A-85380, which was developed as a single-photon emission computed tomography agent for the non-invasive study of α4β2 nAChR in the brain. On the other hand, there are some implications that homomeric α7 nAChRs may play a role in the pathophysiology of neuropsychiatric disorders (7-9). α7 nAChRs are highly expressed in the cerebral cortex, hippocampus, and subcortical limbic regions, which are involved in learning, memory, and information processing (10-12). 4-Bromophenyl-1,4-diazabicyclo(3.2.2)nonane-4-carboxylate (SSR180711) has been shown to be a potent and selective partial agonist for α7 nAChRs with nanomolar affinity (13). 4-[^11^C]Methylphenyl-1,4-diazabicyclo(3.2.2)nonane-4-carboxylate ([^11^C]CHIBA-1001) has been developed as a PET agent for the noninvasive study of α7 nAChR in the brain (14). In this chapter, another α7 nAChR agonist, 2-(5-[^11^C]methyl-hexahydro-pyrrolo[3,4-c]pyrrol-2-yl)-xanthene-9-one ([^11^C]A-844606) (15), is being evaluated as a useful PET imaging agent.

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=nicotinic%20acetylcholine%20receptor+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Gene information in NCBI (α7 nAChR (http://www.ncbi.nlm.nih.gov/gene/1139))
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/omim/118511)
- Clinical trials (α7 nAChR (http://www.clinicaltrials.gov/ct2/results?term=alpha+7+nicotinic+cholinergic+receptors))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=A-844606%20and%20synthesis)]

Toyohara et al. (15) reported the synthesis of [^11^C]A-844606 by methylation of desmethyl-A-844606 in the presence of NaOH with [^11^C]methyl triflate in an automated synthesis system. The mixture was allowed to react for 1 min at room temperature, and [^11^C]A-844606 was purified with high-performance liquid chromatography (HPLC). Average radiochemical yield was 40.0 ± 16.8% (n = 7). The radiochemical purity was >97% with a specific activity of 15–108 GBq/µmol (0.4–3.0 Ci/µmol) at the end of synthesis. Total synthesis time was ~30 min from the end of bombardment.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=A-844606%20and%20in%20vitro)]

Briggs et al. (16) reported that A-844606 exhibited an IC_50_ value of 11 nM for α7 nAChRs (obtained with the use of [^3^H]methyllycaconitine) in rat brain membranes. A-844606 exhibited little affinity for α4β2 nAChRs.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=A-844606%20and%20rodentia)]

Toyohara et al. (15) performed ex vivo biodistribution of 2 MBq (0.054 mCi) [^11^C]A-844606 (0.05 nmol) in normal mice (n = 4/group) at 1–60 min. The highest uptake (percentage of injected dose per gram of tissue (% ID/g)) of [^11^C]A-844606 was found in the lungs (45.9), followed by the kidneys (12.37), small intestines (9.6), heart (9.3), brain (8.0), pancreas (7.8), liver (7.6), spleen (7.3), and muscle (2.5) at 1–30 min after injection. The radioactivity level of [^11^C]A-844606 in the blood was low (0.6) at 5 min after injection. HPLC analysis of the plasma showed that 40.0% and 28.9% of [^11^C]A-844606 were intact at 15 min and 30 min after injection with two major hydrophilic metabolites. On the other hand, little degradation of [^11^C]A-844606 was detected in the brain (>95% intact) at these time points. Blocking studies were performed with co-injection (1 mg/kg) of the selective α7 nAChR agonists (SSR180711, A-582941, A-844606) and the selective α4β2 nAChR agonist A-85380 at 15 min after injection. In the control mice, accumulation in the hippocampus, medulla oblongata, hypothalamus, striatum, midbrain, and cerebral cortex was not significantly higher than accumulation in the cerebellum indicating high level of non-specific binding of [^11^C]A-844606. SSR180711, A-582941, and A-85380 did not significantly decrease the accumulation of [^11^C]A-844606 in the brain tissues, whereas A-844606 inhibited the accumulation of [^11^C]A-844606 in all brain regions by 40%–50% (P < 0.05).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=A-844606%20and%20(dog%20or%20pig%20or%20sheep%20or%20rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=A-844606%20and%20(primate%20not%20human))]

[^11^C]A-844606 PET studies with rhesus monkeys (n = 3) showed substantial brain accumulation with selective uptake in the regions of the hippocampus, frontal cortex, thalamus, and cerebellum at 10–30 min after injection with gradual washouts (15). In Logan graphical analysis (total distribution volume (V_T_)), the cerebellum (95.2 ± 32.8 ml/g) showed lower binding than the hippocampus (118.5 ± 33.6 ml/g), frontal cortex (130.9 ± 40.4 ml/g), and thalamus (138.6 ± 42.3 ml/g). The regional distribution of [^11^C]A-844606 is consistent with the distribution of α7 nAChRs. [^11^C]A-844606 V_T_ values in the brain regions were reduced by ~50% with pretreatment with SSR180711 (5.0 mg/kg, 30 min). The fractions of unchanged [^11^C]A-844606 in the plasma at 1 min and 30 min after injection as determined with thin-layer chromatography were 69% and 28%, respectively. Detection of specific binding in the conscious monkeys (PET scans) and not in mice (ex vivo biodistribution) may be explained by the differences in species and blocking experiments (co-injection in mice versus pretreatment in monkeys).

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=A-844606%20and%20human)]

No publication is currently available.

## References

1 Alkondon M., Albuquerque E.X. (2004). The nicotinic acetylcholine receptor subtypes and their function in the hippocampus and cerebral cortex. Prog Brain Res.
2 Gotti C., Riganti L., Vailati S., Clementi F. (2006). Brain neuronal nicotinic receptors as new targets for drug discovery. Curr Pharm Des.
3 Hogg R.C., Raggenbass M., Bertrand D. (2003). Nicotinic acetylcholine receptors: from structure to brain function. Rev Physiol Biochem Pharmacol.
4 Abreo M.A., Lin N.H., Garvey D.S., Gunn D.E., Hettinger A.M., Wasicak J.T., Pavlik P.A., Martin Y.C., Donnelly-roberts D.L., Anderson D.J., Sullivan J.P., Williams M., Arneric S.P., Holladay M.W. (1996). Novel 3-Pyridyl ethers with subnanomolar affinity for central neuronal nicotinic acetylcholine receptors. J Med Chem.
5 Sullivan J.P., Donnelly-Roberts D., Briggs C.A., Anderson D.J., Gopalakrishnan M., Piattoni-Kaplan M., Campbell J.E., McKenna D.G., Molinari E., Hettinger A.M., Garvey D.S., Wasicak J.T., Holladay M.W., Williams M., Arneric S.P. (1996). A-85380 [3-(2(S)-azetidinylmethoxy) pyridine]: in vitro pharmacological properties of a novel, high affinity alpha 4 beta 2 nicotinic acetylcholine receptor ligand. Neuropharmacology.
6 Akerman M.E., Pilch J., Peters D., Ruoslahti E. (2005). Angiostatic peptides use plasma fibronectin to home to angiogenic vasculature. Proc Natl Acad Sci U S A.
7 Gotti C., Zoli M., Clementi F. (2006). Brain nicotinic acetylcholine receptors: native subtypes and their relevance. Trends Pharmacol Sci.
8 Nomikos G.G., Schilstrom B., Hildebrand B.E., Panagis G., Grenhoff J., Svensson T.H. (2000). Role of alpha7 nicotinic receptors in nicotine dependence and implications for psychiatric illness. Behav Brain Res.
9 Nordberg A. (2001). Nicotinic receptor abnormalities of Alzheimer's disease: therapeutic implications. Biol Psychiatry.
10 Thomsen M.S., Hansen H.H., Timmerman D.B., Mikkelsen J.D. (2010). Cognitive improvement by activation of alpha7 nicotinic acetylcholine receptors: from animal models to human pathophysiology. Curr Pharm Des.
11 Barrantes F.J., Borroni V., Valles S. (2010). Neuronal nicotinic acetylcholine receptor-cholesterol crosstalk in Alzheimer's disease. FEBS Lett.
12 Hajos M., Rogers B.N. (2010). Targeting alpha7 nicotinic acetylcholine receptors in the treatment of schizophrenia. Curr Pharm Des.
13 Biton B., Bergis O.E., Galli F., Nedelec A., Lochead A.W., Jegham S., Godet D., Lanneau C., Santamaria R., Chesney F., Leonardon J., Granger P., Debono M.W., Bohme G.A., Sgard F., Besnard F., Graham D., Coste A., Oblin A., Curet O., Vige X., Voltz C., Rouquier L., Souilhac J., Santucci V., Gueudet C., Francon D., Steinberg R., Griebel G., Oury-Donat F., George P., Avenet P., Scatton B. (2007). SSR180711, a novel selective alpha7 nicotinic receptor partial agonist: (1) binding and functional profile. Neuropsychopharmacology.
14 Hashimoto K., Nishiyama S., Ohba H., Matsuo M., Kobashi T., Takahagi M., Iyo M., Kitashoji T., Tsukada H. (2008). [11C]CHIBA-1001 as a novel PET ligand for alpha7 nicotinic receptors in the brain: a PET study in conscious monkeys. PLoS ONE.
15 Toyohara J., Ishiwata K., Sakata M., Wu J., Nishiyama S., Tsukada H., Hashimoto K. (2010). In vivo evaluation of alpha7 nicotinic acetylcholine receptor agonists [11C]A-582941 and [11C]A-844606 in mice and conscious monkeys. PLoS ONE.
16 Briggs C.A., Schrimpf M.R., Anderson D.J., Gubbins E.J., Gronlien J.H., Hakerud M., Ween H., Thorin-Hagene K., Malysz J., Li J., Bunnelle W.H., Gopalakrishnan M., Meyer M.D. (2008). alpha7 nicotinic acetylcholine receptor agonist properties of tilorone and related tricyclic analogues. Br J Pharmacol.